# Gadolinium-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-icosahedral closo-borane_12_ scaffold conjugated with Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-icosahedral closo-borane_12_ scaffold conjugated with Glu-{Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_
Abbreviated name: | CA-12
Synonym: | Gd-DOTA-closo-B_12_-E-{E-[c(RGDfK)]_2_}_2_
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally (1). Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field. Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images (2). Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (3, 4). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (5). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (6-10). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (8-12). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for the imaging of tumors and tumor angiogenesis (13).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (14) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in xenografts in nude mice (15, 16). Several small molecular MRI Gd-based contrast agents conjugated with a cyclic RGD peptide have been studied (17). However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, these low molecular weight MRI contrast agents exhibit low r_1_ relaxivity value (~4 mM^–1^s^–1^ per Gd) and high toxicity (nephrogenic systemic fibrosis in patients with renal dysfunction) (18). In order to obtain sufficient contrast enhancement, a large number of Gd^3+^ ions bound per target is needed. Li et al. (19) have developed polyhedral boranes as a scaffold for the targeted high payload delivery of drugs and imaging agents. A functionalizable monodisperse molecular borane scaffold, [closoB_12_(OH)_12_]^2–^, conjugated with twelve radial ethylene glycol (PEG)_3_ arms with attachments of Gd-chelates (20). Goswami et al. (21) utilized [closoB_12_(OH)_12_]^2–^ as a high payload MRI contrast agent (CA-12) carrying eleven copies of Gd-DOTA chelates and one copy of Glu-Glu-{[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_}_2_ (cRGD) via PEG linkers for use as a high-performance MRI contrast agent in nude mice bearing human breast cancer xenografts.

### Related Resource Links:

- Chapters in MICAD (Gd (http://www.ncbi.nlm.nih.gov/books/?term=Gadolinium+AND+micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+synthesis)]

The 12-fold carbamate closomer 5 was reacted with amino-terminated DOTA-(PEG)_5_ ligand 4 to form 12-fold DOTA-conjugated closomer 6 with 80% yield (21). Closomer 6 was isolated with column chromatography and then treated with trifluoroacetic acid (TFA) to remove the tert-butyl ester protecting groups. The deprotected closomer 6 was incubated with GdCl_3_ in a citrate buffer (pH 7) to provide closomer CA-7 with 71% yield. CA-7 was purified with dialysis in ultrapure water. There were 11.4 Gd^3+^ ions per CA-7 as measured with inductively coupled plasma optical emission spectroscopy (ICP-OES). The average CA-7 particle diameter was 10 nm as measured with dynamic laser scattering (DLS).

The 11-fold carbonate closomer 9 with an azido-terminated (PEG)_8_ linker was reacted with alkyne-terminated (PEG)_9_ cRGD peptide by an azide-alkyne click reaction (21). The resulting cRGD-closomer 10 was isolated with column chromatography. DOTA ligands were added to the remaining 11 vertices by reaction with amino-terminated DOTA-(PEG)_5_ ligand 4 to obtain the 11-fold carbamate closomer 11 in 83% yield. Closomer 11 was isolated with column chromatography and then treated with TFA to remove the tert-butyl ester protecting groups. The deprotected closomer 11 was incubated with GdCl_3_ in a citrate buffer (pH 7) to provide closomer CA-12 with 69% yield. CA-12 was purified with dialysis in ultrapure water. There were 10.6 Gd^3+^ ions per CA-12 as measured with ICP-OES. The average CA-12 particle diameter was 12–13 nm as measured with DLS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+in+vitro)]

CA-7 exhibited an r_1_ value (7 T) of 4.8 mM^–1^s^–1^ per Gd in phosphate-buffered saline (PBS) to provide a molar relaxivity value of 54.7 mM^–1^s^–1^ (21). CA-12 exhibited an r_1_ value of 5.9 mM^–1^s^–1^ per Gd to provide a molar relaxivity value of 62.5 mM^–1^s^–1^. Omniscan (Gd-DTPA-BMA) had a molar relaxivity value of 4.2 mM^–1^s^–1^. Cellular accumulation of CA-12 was performed by incubation of CA-9 (5 mM Gd) with MDA-MB-231 (α_v_β_3_-positive) and T47D (α_v_β_3_-negative) cells for 30 min at 37°C. The Gd concentration was 200% higher in MDA-MB-231 cells (90 µg Gd/g cell lysate) than in T47D cells (30 µg Gd/g cell lysate). No blocking studies were performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+rodentia)]

Goswami et al. (21) performed dynamic T1-weighted MRI (7 T) studies with intravenous injection of 0.04 mmol Gd/kg CA-12, CA-7, or Gd-DTPA-BMA in nude mice (n = 6/group) bearing PC-3 xenografts. Contrast-enhanced MRI signal intensity (SI) levels were obtained at 1 min, 30 min, 1 h, 4 h, and 24 h after intravenous injection. Enhanced contrast in the tumor tissues was visualized for CA-12 for up to 4 h, whereas contrast enhancement with CA-7 persisted for only 1 h after injection. On the other hand, Gd-DTPA-BMA exhibited contrast enhancement within 30 min, and little enhancement was detected after 1 h. Contrast enhancement ratios (CERs) [CER = (SI_post_ – SI_pre_)/SI_pre_ X 100%] for CA-12 were 16%, 27%, 24%, 17%, and 3% at 1 min, 30 min, 1 h, 4 h, and 24 h, respectively. CERs for CA-7 were 13%, 18%, 16%, 10%, and 3% at 1 min, 30 min, 1 h, 4 h, and 24 h, respectively. The CERs of tumors for Gd-DTPA-BMA were 32%, 18%, 4%, 4%, and 3% at 1 min, 30 min, 1 h, 4 h, and 24 h, respectively. At 1 h and 4 h after injection of CA-12, tumor tissues exhibited significant higher CERs compared to those with CA-7 (P < 0.01 at 1 h) and Gd-DTPA-BMA (P < 0.01 at 1 h, P < 0.05 at 4 h). The three agents showed high CERs of 90%–120% in the kidneys at 1 min, which declined to ~3% at 24 h. CERs for CA-12 and CA-7 declined more slowly than that for Gd-DTPA-BMA. The Gd contents in the kidneys as well as other major normal tissues were not detectable for the three agents by 24 h after injection. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cRGD%20CA-12+human)]

No publication is currently available.

## NIH Support

R21 CA114090

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Burtea, C., S. Laurent, L. Vander Elst, and R.N. Muller, Contrast agents: magnetic resonance. Handb Exp Pharmacol, 2008(185 Pt 1): p. 135-65.
3 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
4 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
5 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
6 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
7 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
8 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
9 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
12 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
13 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
14 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
15 Beer A.J., Kessler H., Wester H.J., Schwaiger M. (2011). PET Imaging of Integrin alphaVbeta3 Expression. Theranostics.
16 Zhou Y., Chakraborty S., Liu S. (2011). Radiolabeled Cyclic RGD Peptides as Radiotracers for Imaging Tumors and Thrombosis by SPECT. Theranostics.
17 Tan M., Lu Z.R. (2011). Integrin Targeted MR Imaging. Theranostics.
18 Laurent S., Elst L.V., Muller R.N. (2006). Comparative study of the physicochemical properties of six clinical low molecular weight gadolinium contrast agents. Contrast Media Mol Imaging.
19 Li T., Jalisatgi S.S., Bayer M.J., Maderna A., Khan S.I., Hawthorne M.F. (2005). Organic syntheses on an icosahedral borane surface: closomer structures with twelvefold functionality. J Am Chem Soc.
20 Goswami L.N., Ma L., Chakravarty S., Cai Q., Jalisatgi S.S., Hawthorne M.F. (2013). Discrete nanomolecular polyhedral borane scaffold supporting multiple gadolinium(III) complexes as a high performance MRI contrast agent. Inorg Chem.
21 Goswami L.N., Ma L., Cai Q., Sarma S.J., Jalisatgi S.S., Hawthorne M.F. (2013). cRGD peptide-conjugated icosahedral closo-B12(2-) core carrying multiple Gd3+-DOTA chelates for alpha(v)beta3 integrin-targeted tumor imaging (MRI). Inorg Chem.